# Cy5.5-Chitosan-anti-vascular endothelial growth factor receptor 2 monoclonal antibody DC101

Chemical name: | Cy5.5-Chitosan-anti-vascular endothelial growth factor receptor 2 monoclonal antibody DC101
Abbreviated name: | Cy5.5-Chitosan-DC101
Synonym:
Agent category: | Antibody
Target: | Vascular endothelial growth factor receptor 2 (VEGFR-2)
Target category: | Receptor
Method of detection: | Optical imaging, near-infrared red (NIR) fluorescence imaging
Source of signal/contrast: | Cy5.5
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=9087218), nucleotide (http://www.ncbi.nlm.nih.gov/nuccore/229892299) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=Graphics&list_uids=3791) for more information about VEGFR-2.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=DC101%20chitosan)]

Vascular endothelial growth factor (VEGF) consists of at least six isoforms with various numbers of amino acids (121, 145, 165, 183, 189, and 206 amino acids) produced through alternative splicing (1). VEGF_121_, VEGF_165_, and VEGF_189_ are the forms secreted by most cell types and are active as homodimers linked by disulfide bonds. VEGF_121_ does not bind to heparin like the other VEGF species (2). VEGF is a potent angiogenic factor that induces proliferation, sprouting, migration, and tube formation of endothelial cells. There are three high-affinity tyrosine kinase VEGF receptors (VEGFRs) on endothelial cells (VEGFR-1, Flt-1; VEGFR-2, KDR/Flt-1; and VEGFR-3, Flt-4). Several types of non-endothelial cells such as hematopoietic stem cells, melanoma cells, monocytes, osteoblasts, and pancreatic β cells also express VEGFRs (1).

VEGFRs have been found to be overexpressed in various tumor cells and tumor-associated endothelial cells (3). Inhibition of VEGFR function has been shown to inhibit pathological angiogenesis as well as tumor growth and metastasis (4, 5). Radiolabeled VEGF has been developed as a tracer for imaging solid tumors and angiogenesis in humans (6-8). Chitosan (5 kDa) is a linear polysaccharide composed of D-glucosamine and N-acetylglucosamine subunits with numerous amine groups of D-glucosamine for ligand conjugation. A rat anti-VEGFR-2 monoclonal antibody (mAb), DC101, has been shown to inhibit angiogenesis with suppression of tumor growth and metastasis. Lee et al. (9) conjugated chitosan to DC101 mAb for labeling with Cy5.5 to form Cy5.5-chitosan-DC101 for NIR fluorescence imaging of VEGFR-2 expression under ischemic conditions.

### Related Resource Links:

- Chapters in MICAD (VEGFR (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=VEGFR+AND+micad%5Bbook%5D), DC101 (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=DC101+AND+micad%5Bbook%5D))
- Gene information in NCBI (VEGFR (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=DetailsSearch&Term=3791))
- Articles in Online Mendelian Inheritance in Man (OMIM) (VEGFR (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=omim&Cmd=DetailsSearch&Term=VEGFR))
- Clinical trials (VEGFR (http://www.clinicaltrials.gov/ct2/results?term=VEGFR))
- FDA Drug information (VEGFR (http://google2.fda.gov/search?q=VEGFR&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=12&y=7))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=DC101%20chitosan+synthesis)]

DC101 mAb (6.6 nM) was incubated with 20 mM sodium meta-periodate for 30 min at 4°C (9). The periodate-oxidized mAb and chitosan were incubated in the presence of sodium cynoborohydride for 2 h at 4°C. Chitosan-DC101 and chitosan-IgG conjugates were isolated with ultracentrifugation. The molecular weights of DC101 and chitosan-DC101 were found with MALDI-TOF mass spectroscopy to be 144.7 and 150.6 kDa, respectively. Hence, there was approximately one chitosan moiety per antibody. Cy5.5-chitosan-DC101 was prepared by incubation of Cy5.5-NHS and chitosan-CD101 for 20 h at room temperature. Cy5.5-Chitosan-DC101 conjugates were isolated with column chromatography. The number of Cy5.5 molecules per antibody was not reported. Cy5.5-Chitosan-IgG conjugates were also prepared similarly.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=DC101%20chitosan+in+vitro)]

In vitro binding tests showed binding of FITC-chitosan-DC101 (0.13 nmol) to human umbilical vein endothelial cells (HUVECs) expressing VEGFR-2. Confocal microscopy showed that most of the FITC-chitosan-DC101 bound to the cytosol of HUVECs after 2 h of incubation (9). In contrast, FITC-chitosan-IgG control did not bind to the cells. Flow cytometry analysis showed that FITC-chitosan-DC101 binding to the cells exhibited ~10-fold greater fluorescent intensity than FITC-chitosan-IgG binding.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=DC101%20chitosan+rodentia)]

Lee et al. (9) performed optical imaging using an ischemic mouse model. Images were captured at 3 h after intravenous injection of Cy5.5-chitosan-DC101 at 12, and 24 h after artery ligation. The accumulation of fluorescence signal in the ischemic hindlimb was higher than the hindlimb at 12 h after operation and continued to increase at 24 h after operation. On the other hand, the Cy5.5-chitosan-IgG control did not show any significant accumulation in the ischemic and contralateral hindlimbs. There was an increase of VEGFR-2 expression with time in the ischemic tissues. No blocking experiment was performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=DC101%20chitosan+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=DC101%20chitosan+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=DC101%20chitosan+human)]

No publication is currently available.

## References

1 Ferrara N. (2004). Vascular endothelial growth factor: basic science and clinical progress. Endocr Rev.
2 Cohen T., Gitay-Goren H., Sharon R., Shibuya M., Halaban R., Levi B.Z., Neufeld G. (1995). VEGF121, a vascular endothelial growth factor (VEGF) isoform lacking heparin binding ability, requires cell-surface heparan sulfates for efficient binding to the VEGF receptors of human melanoma cells. J Biol Chem.
3 Soria J.C., Fayette J., Armand J.P. (2004). Molecular targeting: targeting angiogenesis in solid tumors. Ann Oncol.
4 Ferrara N. (2004). Vascular endothelial growth factor as a target for anticancer therapy. Oncologist.
5 Hicklin D.J., Ellis L.M. (2005). Role of the vascular endothelial growth factor pathway in tumor growth and angiogenesis. J Clin Oncol.
6 Li S., Peck-Radosavljevic M., Koller E., Koller F., Kaserer K., Kreil A., Kapiotis S., Hamwi A., Weich H.A., Valent P., Angelberger P., Dudczak R., Virgolini I. (2001). Characterization of (123)I-vascular endothelial growth factor-binding sites expressed on human tumour cells: possible implication for tumour scintigraphy. Int J Cancer.
7 Li S., Peck-Radosavljevic M., Kienast O., Preitfellner J., Hamilton G., Kurtaran A., Pirich C., Angelberger P., Dudczak R. (2003). Imaging gastrointestinal tumours using vascular endothelial growth factor-165 (VEGF165) receptor scintigraphy. Ann Oncol.
8 Li S., Peck-Radosavljevic M., Kienast O., Preitfellner J., Havlik E., Schima W., Traub-Weidinger T., Graf S., Beheshti M., Schmid M., Angelberger P., Dudczak R. (2004). Iodine-123-vascular endothelial growth factor-165 (123I-VEGF165). Biodistribution, safety and radiation dosimetry in patients with pancreatic carcinoma. Q J Nucl Med Mol Imaging.
9 Lee, C.M., E.M. Kim, S.J. Cheong, D.W. Kim, S.T. Lim, M.H. Sohn, and H.J. Jeong, Targeted molecular imaging of VEGF receptors overexpressed in ischemic microvasculature using chitosan-DC101 conjugates. J Biomed Mater Res A, 2009